# [^18^F]-5-(2-fluoroethyl)2,4-diethyl-3-(ethylsulfanylcarbonyl)-6-phenylpyridine-5-carboxylate

Chemical name: | [^18^F]-5-(2-fluoroethyl)2,4-diethyl-3-(ethylsulfanylcarbonyl)-6-phenylpyridine-5-carboxylate
Abbreviated name: | [^18^F]FE@SUPPY
Synonym:
Agent Category: | Compound
Target: | Adenosine A_3_ receptors
Target Category: | Receptor-ligand binding
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information regarding [^18^F]FE@SUPPY in PubChem (http://pubchem.ncbi.nlm.nih.gov/). See (1) for the structure and other information regarding [^18^F]FE@SUPPY:2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=adenosine%20receptors&cmd=DetailsSearch)]

Adenosine is an important signaling molecule that is involved in several pathophysiological conditions such as asthma, inflammation, and neurodegeneration. It is known to mediate its effects through four G-protein–coupled receptors, A_1_, A_2_ (with sub types A_2A_ and A_2B_), and A_3_ (the receptors are also designated as A1AR, A2AR, and A3AR, respectively) in the mammalian system. These receptors have been identified in several human tissues and, because they play a role in different pathologies, are targeted for the clinical development of a variety of drugs (2, 3). Much information is available regarding the function and tissue distribution of the A_1_ and A_2A_ receptors; however, because of a lack of proper agonists and antagonists to study the A_2B_ and A_3_ receptors, the exact role of the latter two receptors in mammalian physiology is not clear (4). In addition to its possible involvement in the development of rheumatoid arthritis and brain, lung, and cardiac ischemia, the A_3_ receptor was shown to be overexpressed and had a proliferative effect in certain cancer tissues and cell lines (5-7). Although this receptor is known to be involved in a number of diseases, little is known about its expression and distribution in the different regions and tissue of the body (4).

In an attempt to study the ligand binding properties of the A_3_ receptor, investigators developed antagonistic pyridine analogs that showed high affinity and specificity for the receptor (8, 9). Among these pyridine compounds, a fluoroethyl ester derivative, 5-(2-fluoroethyl)2,4-diethyl-3-(ethylsulfanylcarbonyl)-6-phenylpyridine-5-carboxylate (FE@SUPPY), was determined to have a high affinity and selectivity for the A_3_ receptor (9). Recently, Wadsak et al. developed a suitable precursor for the synthesis of FE@SUPPY and labeled the A_3_ ligand with radioactive fluorine (^18^F) to obtain [^18^F]FE@SUPPY (4). The labeled compound was subsequently studied for its biodistribution in rats and its specificity was determined by autoradiography.

The metabolic properties of [^18^F]FE@SUPPY were compared to those of its analogue, [^18^F]FE@SUPPY:2 (5-ethyl-2,4-diethyl-3-((2-[^18^F]fluoroethylsulfanylcarbonyl)-6-phenylpyridine-5-carboxylate), in rodents by Haeusler et. al. (1). To compare the structures of [^18^F]FE@SUPPY and [^18^F]FE@SUPPY:2 see (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FE@SUPPY%20synthesis&cmd=DetailsSearch)]

5-(2-Tosyloxyethyl)2,4-diethyl-3-(ethylsulfanylcarbonyl)-6-phenylpyridine-5-carboxylate (Tos@SUPPY), the precursor of [^18^F]FE@SUPPY, was synthesized from 5-(2-oxyethyl)2,4-diethyl-3-(ethylsulfanylcarbonyl)-6-phenylpyridine-5-carboxylate (OH@SUPPY) as described by Wadsak et al. (4). Briefly, OH@SUPPY and triethylamine were mixed with a solution of toluene-4-sulfonyl chloride in trihydrofluoric acid at 0°c and refluxed for 62 h. The mixture was then dried under a vacuum, and Tos@SUPPY was recrystallized from diethyl ether.

For the radiosynthesis of [^18^F]FE@SUPPY, ^18^F was eluted from a carbonate form of an anion exchange cartridge with an acetonitrile/water mixture containing 4,7,13,16,21,24-hexaoxo-1,10-diaza-bicyclo[8.8.8]hexacosane and potassium bicarbonate (4). This mixture was heated to 100°C and dried azeotropically in a stream of nitrogen gas to obtain a ^18^F-labeled fluoride-aminopolyether complex. Subsequently, Tos@SUPPY in acetonitrile was added to the dried and labeled polyether, and the solution was heated to 75°C for 20 min. The reaction was stopped by the addition of water, and the product was loaded onto a semipreparative, reverse-phase, high-performance liquid chromatography (HPLC) column. Fractions containing the radiolabeled compound were collected and loaded on a C18plus Sep-Pak column. The column was washed with water and [^18^F]FE@SUPPY was then eluted in ethanol, sterile-filtered with a 0.22-μm filter, and reformulated in normal saline (4).

Radiochemical purity (RP) of the labeled product was always >98% (n = 13 batches) as determined by thin-layer chromatography (TLC) and HPLC. On the basis of ^18^F (corrected for decay), the product yield of the reaction was 35 ± 15%, with a specific activity of 66 ± 20 GBq/μmol (1.78 ± 0.54 Ci/mmol) at the end of synthesis (4). Using TLC the stability of [^18^F]FE@SUPPY was reported to be at least 10 h after synthesis.

In some studies [^18^F]FE@SUPPY:2 was used for comparison purposes and the automated synthesis of this radiocompound is described elsewhere (1). This tracer had a specific activity of 340 ± 140 GBq/μmol (9.18 ± 3.78 Ci/μmol) at the end of synthesis with an RP of >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FE@SUPPY%20in%20vitro&cmd=DetailsSearch)]

The preliminary binding study of [^18^F]FE@SUPPY was performed with rat brain slices (4). In the same study, the uptake of [^18^F]FE@SUPPY was also studied in the presence of 1-[2-chloro-6-[[(3-iodophenyl)methyl]amino]-9H-9-yl]-1-deoxy-N-methyl-β-D-ribofuranuronamide) (2-Cl-IB-MECA), a receptor A_3_ antagonist. The specificity of [^18^F]FE@SUPPY for the A_3_ receptor was established because it was displaced by 2-Cl-IB-MECA in the blocking experiment (4). However, although the investigators used autoradiography to establish that the radiochemical was incorporated primarily in the nucleus accumbens and caudate putamen regions of the brain, with little uptake in the cortical regions, this technique could not establish definite specificity of the radioligand for the A_3_ receptor in these regions (4).

Using an in vitro porcine carboxylestrase assay the Michaelis-Menten constants for [^18^F]FE@SUPPY and [^18^F]FE@SUPPY:2 were reported to be 20.15 and 13.11 μM, respectively (1). The limiting velocities of the reaction were 0.035 and 0.015 μM/min, respectively, for the two compounds.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18%20F%20FE@SUPPY%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]FE@SUPPY was studied in normal Sprague-Dawley rats after injecting the agent into the animals through the tail vein (4). The animals were then euthanized at various time points (n = 4 rats per time point) between 5 and 120 min after injection; the organs were removed, dry-weighed, and counted for incorporated radioactivity. The complete biodistribution of [^18^F]FE@SUPPY is given in Table 1 of Wadsak et al. (4). The tissue/blood ratios (TBR) for [^18^F]FE@SUPPY uptake by the various organs are given in Figure 3 of Wadsak et al. (4). On the basis of the TBR, highest uptake was observed in the liver at 15 min: 1.87 ± 0.16 percent of the injected dose per gram of tissue weight (% ID/g), which decreased to 1.41 ± 0.57% ID/g at 30 min. A high incorporation of [^18^F]FE@SUPPY was also observed in the kidneys, lungs, and heart, but the level of uptake in these organs was moderate compared to the liver. The investigators reported an intermediate uptake of the radiochemical (0.2–0.33% ID/g) in the brain, and the blood level remained at 0.04 ± 0.09% ID/g during the entire study. The investigators reported that there was an agreement between the A_3_ receptor mRNA expression and biodistribution of [^18^F]FE@SUPPY in the various organs of the animals (4, 10).

In an in vivo study with rats 47.7% and 30.3% of [^18^F]FE@SUPPY was intact (as determined by HPLC) in the blood at 15 and 30 min post injection (p. i.), respectively, and only 33.1% and 15.6% of [^18^F]FE@SUPPY:2 was reported to be intact at the two time points, respectively (1). In the brain [^18^F]FE@SUPPY:2 was metabolized quickly, however [^18^F]FE@SUPPY metabolites were observed in this organ only 30 min p. i. indicating that this radiochemical was degraded slowly compared to its analogue. From this study the investigatots concluded that [^18^F]FE@SUPPY was probably more suitable than [^18^F]FE@SUPPY:2 for evaluation in a clinical investigation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fe@suppy%20non%20primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fe@suppy%20non%20human%20primate&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fe@suppy%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Haeusler D., Nics L., Mien L.K., Ungersboeck J., Lanzenberger R.R., Shanab K., Sindelar K.M., Viernstein H., Wagner K.H., Dudczak R., Kletter K., Wadsak W., Mitterhauser M. (2010). [18F]FE@SUPPY and [18F]FE@SUPPY:2--metabolic considerations. Nucl Med Biol.
2 Gao Z.G., Jacobson K.A. (2007). Emerging adenosine receptor agonists. Expert Opin Emerg Drugs.
3 Gessi S., Merighi S., Varani K., Leung E., Mac Lennan S., Borea P.A. (2008). The A(3) adenosine receptor: An enigmatic player in cell biology. Pharmacol Ther.
4 Wadsak W., Mien L.K., Shanab K., Ettlinger D.E., Haeusler D., Sindelar K., Lanzenberger R.R., Spreitzer H., Viernstein H., Keppler B.K., Dudczak R., Kletter K., Mitterhauser M. (2008). Preparation and first evaluation of [(18)F]FE@SUPPY: a new PET tracer for the adenosine A(3) receptor. Nucl Med Biol.
5 Chen G.J., Harvey B.K., Shen H., Chou J., Victor A., Wang Y. (2006). Activation of adenosine A3 receptors reduces ischemic brain injury in rodents. J Neurosci Res.
6 Gessi S., Merighi S., Varani K., Cattabriga E., Benini A., Mirandola P., Leung E., Mac Lennan S., Feo C., Baraldi S., Borea P.A. (2007). Adenosine receptors in colon carcinoma tissues and colon tumoral cell lines: focus on the A(3) adenosine subtype. J Cell Physiol.
7 Madi L., Cohen S., Ochayin A., Bar-Yehuda S., Barer F., Fishman P. (2007). Overexpression of A3 adenosine receptor in peripheral blood mononuclear cells in rheumatoid arthritis: involvement of nuclear factor-kappaB in mediating receptor level. J Rheumatol.
8 Xie R., Li A.H., Ji X.D., Melman N., Olah M.E., Stiles G.L., Jacobson K.A. (1999). Selective A(3) adenosine receptor antagonists: water-soluble 3, 5-diacyl-1,2,4-trialkylpyridinium salts and their oxidative generation from dihydropyridine precursors. J Med Chem.
9 Li A.H., Moro S., Forsyth N., Melman N., Ji X.D., Jacobson K.A. (1999). Synthesis, CoMFA analysis, and receptor docking of 3,5-diacyl-2, 4-dialkylpyridine derivatives as selective A3 adenosine receptor antagonists. J Med Chem.
10 Fredholm B.B., Arslan G., Halldner L., Kull B., Schulte G., Wasserman W. (2000). Structure and function of adenosine receptors and their genes. Naunyn Schmiedebergs Arch Pharmacol.